# [^18^F]Fluorobenzyl-bombesin[7-14]-c(RGDyK)

Chemical name: | [^18^F]Fluorobenzyl-bombesin[7-14]-c(RGDyK)
Abbreviated name: | [^18^F]FB-BBN-c(RGDyK)
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptors (GRPR), integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on CNS and GI tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (12, 14, 15). A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (16).

Because prostate cancer expresses both GRPR and α_v_β_3_, Li et al. (17) designed a BBN-RGD heterodimer in which BBN[7-14] and c(RGDyK) were connected with a glutamate linker. N-Succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) was used to synthesize [^18^F]FB-BBN-RGD for tumor targeting.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+synthesis)]

[^18^F]SFB was added to a solution of 100 nmol BBN-RGD (17). The mixture was heated for 30 min at 60°C. The product, [^18^F]FB-BBN-RGD, was purified with high-performance liquid chromatography with a decay-corrected yield of 12.0 ± 0.7% (n = 4) based on [^18^F]SFB and a radiochemical purity of >99%. [^18^F]FB-BBN and [^18^F]FB-RGD were synthesized using the same procedure. The specific activities of [^18^F]FB-BBN-RGD, [^18^F]FB-BBN, and [^18^F]FB-RGD were estimated to be ~100 MBq/nmol (2.7 mCi/nmol). The log P values were -0.92, 1.49, and -1.75 for [^18^F]FB-BBN-RGD, [^18^F]FB-BBN, and [^18^F]FB-RGD, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+in+vitro)]

Li et al. (17) performed in vitro inhibition studies of RGD, BBN-RGD, and FB-BBN-RGD in cultured U87MG cells with ^125^I-echistatin for α_v_β_3_ integrin binding. The 50% inhibition concentration (IC_50_) values were 202, 428, and 282 nM, respectively. In vitro inhibition studies of BBN, BBN-RGD, and FB-BBN-RGD were also performed in cultured PC-3 cells with ^125^I-BBN for GRPR binding. The IC_50_ values were 20.7, 35.7, and 32 nM, respectively. Therefore, the BBN-RGD heterodimer exhibited comparable binding affinities for α_v_β_3_ integrin with GRPR as the corresponding monomer. PC-3 cells express a high level of GRPR and a moderate level of α_v_β_3_ integrin. PC-3 cells exhibited a 7% and 5% uptake of incubation dose of [^18^F]FB-BBN and [^18^F]FB-BBN-RGD within 30 min of incubation, respectively. On the other hand, PC-3 cells had low uptake of [^18^F]FB-RGD (<0.5%).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+%20rodentia)]

Positron emission tomography analysis was performed after intravenous injection of 3.7 MBq (100 μCi) [^18^F]FB-BBN-RGD, [^18^F]FB-BBN, or [^18^F]FB-RGD in nude mice bearing PC-3 tumors (17). The estimated accumulation of [^18^F]FB-BBN-RGD in the PC-3 tumors was 5.0% injected dose per gram (ID/g) at 30 min and decreased to 3.6% ID/g at 1 h and 2.8% ID/g at 2 h after injection. These tumor uptakes were significantly higher than those for the corresponding monomers and their sum together (P < 0.01). The organs with the highest radioactivity were the kidney and liver. [^18^F]FB-BBN-RGD exhibited higher tumor/organ ratios than the monomers. BBN, c(RGDyK), or BBN+c(RGDyK) were co-injected with [^18^F]FB-BBN-RGD in mice bearing PC-3 tumors. Tumor accumulation at 1 h after injection (3.6% ID/g) was only partially inhibited by either BBN (1.4% ID/g) or RGD (1.8% ID/g) alone. However, BBN+RGD reduced the tumor accumulation to the background level (0.8% ID/g). Even though the α_v_β_3_ integrin expression is weak on PC-3 cells, the specific tumor accumulation of [^18^F]FB-BBN-RGD was strong because of expression of α_v_β_3_ integrin on activated endothelial cells surrounding the PC-3 tumor. Accumulated radioactivity in the bone was low.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+human)]

No publication is currently available.

## NIH Support

R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
15 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
16 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
17 Li Z.B., Wu Z., Chen K., Ryu E.K., Chen X. (2008). 18F-labeled BBN-RGD heterodimer for prostate cancer imaging. J Nucl Med.